# MES-1 F(ab’)_2_ E-selectin monoclonal antibody conjugated to ultrasmall superparamagnetic iron oxide nanoparticle

Chemical name: | MES-1 F(ab’)_2_ E-selectin monoclonal antibody conjugated to ultrasmall superparamagnetic iron oxide nanoparticle
Abbreviated name: | MES-1-USPIO
Synonym:
Agent category: | Antibody fragment
Target: | E-selectin
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20MES-1)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises about 80% of most soft tissues. The contrast of proton MRI depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires development of contrast agents. Most of the contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T-2* is the spin-spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1).

Superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxides particles are coated with a protective layer of dextran or other polysaccharide. These particles have a large combined magnetic moments or spins which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into reticuloendothelial system (RES, #1) is by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (about 20 nm to 3,500 nm in diameters) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles and monocrystalline iron oxide nanoparticles (MION) (1).

USPIO is composed of iron particles of about 4-6 nm and the hydrodynamic diameter is about 20-40 nm. The crystals are covered with a layer of dextran with significant T2 relaxation effects. USPIO has a long plasma half-life due to improved coating. In humans, the blood pool half-life of plasma relaxation times is calculated to about 24 h (2) and 2 h in mice (3). Because of its long blood half-life, USPIO can be used as blood pool agent during the early phase of intravenous administration (4). In the late phase, USPIO is suitable for the evaluation of RES in the body, particularly in lymph nodes (5).

E-selectin is found on the cell surface of endothelial cells (6, 7). It binds to sialy-Lewis^x^ (a carbohydrate moiety) on the cell-surface of leukocytes. Tumor necrosis factor α (TNFα) and interleukin-1 (IL-1), released from inflammatory stimuli, up-regulated E-selectin and other adhesion molecule expression on the vascular endothelial cells leading to leukocyte adhesion to the activated endothelium. E-selectin and other selectins are involved in arresting leukocytes on the endothelium. An anti-E-selectin monoclonal antibody, MES-1 F(ab’)2, was conjugated to USPIO nanoparticles for noninvasive MR imaging of E-selectin expression in inflammation (8).

### Related Resource Links:

- Chapters in MICAD (E-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (E-selectin (http://www.ncbi.nlm.nih.gov/gene/6401)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (E-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D))
- Clinical trials (E-selectin (http://www.clinicaltrials.gov/ct2/results?term=E-selectin))
- Drug information in FDA (E-selectin (http://google2.fda.gov/search?q=e-selectin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20MES-1%20and%20synthesis)]

USPIO nanoparticles (dextran-coated, 30-50 nm) were crosslinked by epichlorohydrin in the presence of sodium hydroxide and then aminated by the addition of 30% ammonia. N-succinimidyl 3-(2-pyridyldithio)propionate (SPDP) was added to the aminated USPIO to form SPDP-USPIO, which was reduced with 15 mg/ml dithiothreitol for 20 minutes. Separately, SPDP was added to antibody (10 mg/ml) at a ratio of 1:100 wt/wt and was incubated for 45 minutes to form SPDP-antibody. To conjugate the antibody to SPDP-USPIO, reduced SPDP-USPIO was incubated with 5 mg of SPDP-antibody overnight. The antibody-labeled USPIO nanoparticles were purified on magnetic columns. The antibodies used were rat anti–mouse E-selectin monoclonal antibody MES-1 F(ab')_2_ and mouse anti–human E-selectin monoclonal antibody F(ab')_2_ 1.2B6 (a non-specific control antibody). Each nanoparticle had about 70 reactive SPDP groups and 13 F(ab’)_2_ molecules.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20MES-1%20and%20in%20vitro)]

Reynolds et al. (8) performed in vitro binding studies by using a Chinese hamster ovary (CHO) cell line stably transfected to express mouse E-selectin. MES-1-USPIO and SPDP-MES-1 exhibited equal binding to the E-selectin on the CHO cells, whereas USPIO nanoparticles showed little binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20MES-1%20and%20rodentia)]

Reynolds et al. (8) used oxazolone to induce contact hypersensitivity by challenging the ears of sensitized mice to produce an inflammatory reaction with erythema and edema. Mean ear thickness increased from 0.30 ± 0.07 mm to 0.83 ± 0.12 mm at 18 h after challenge. The cellular infiltration of leukocytes was clearly detected with hematoxylin-eosin staining. Progressive darkening of the T2 map of challenged ear in mice (n = 6) injected with MES-1–USPIO was observed as a result of the expression of E-selectin on the endothelial cells over the first 48 h. In mice (n = 3) with unchallenged noninflamed ear given MES-1–USPIO or USPIO, no progressive changes were observed. No T2 darkening was observed in the ear of challenged mice (n = 4) with USPIO conjugated with a control antibody F(ab')_2_. Histological analysis confirmed the presence of MES-1-USPIO on both the cell surface and in the cytoplasm of endothelial cells of small to medium sized blood vessels in the inflamed ear.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20MES-1%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20MES-1%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20MES-1%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
3 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
4 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
5 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
6 Bird M.I., Foster M.R., Priest R., Malhotra R. (1997). Selectins: physiological and pathophysiological roles. Biochem Soc Trans.
7 Rosen S.D., Bertozzi C.R. (1994). The selectins and their ligands. Curr Opin Cell Biol.
8 Reynolds P.R., Larkman D.J., Haskard D.O., Hajnal J.V., Kennea N.L., George A.J., Edwards A.D. (2006). Detection of vascular expression of E-selectin in vivo with MR imaging. Radiology.